# Gold nanoparticles

Chemical name: | Gold nanoparticles
Abbreviated name: | AuNPs
Synonym:
Agent category: | Metal
Target: | Non-targeted
Target category: | Non-targeted
Method of detection: | X-ray, CT
Source of signal: | Au
Activation: | No
Studies: | - In vitro; - Rodents | Structure is not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Bismuth%20sulphide%20nanoparticles)]

X-Ray imaging (computed tomography, CT) visualizes tissue density differences that provide the image contrast produced by X-ray attenuation between electron-dense bone and soft tissues (1). Contrast enhancement with use of X-ray contrast (radiopaque) agents are needed to increase the degree of contrast between diseased tissues from normal tissues. Water-soluble X-ray contrast agents are generally based on small tri-iodobenzene compounds as monomers or dimmers (2), which can be ionic (high osmolality) or nonionic (low osmolality). When injected intravenously (intra-arterial catheterization is commonly used), they exhibit highly non-specific vascular permeation and rapid renal excretion limiting their targeting performance.

Gold has not been used as an X-ray contrast agent in vivo. Gold has a higher atomic number and a higher absorption coefficient than iodine, providing 2.7-fold greater contrast/weight than iodine (3). Furthermore, imaging gold at 80-100 keV reduces interference from bone absorption and provides lower soft tissue absorption, which would reduce radiation to patient. Hainfeld et al. (3) have performed experiments in mice using gold nanoparticles (AuNPs, 1.9 nm in diameter, ~50 kDa) as a CT contrast agent. This preparation exhibit excellent stability, high X-ray absorption, good safety profile, long blood half-life, and enhanced CT contrast of the vasculature, kidneys and tumor in mice.

### Related Resource Links:

- Chapters in MICAD (Gold imaging (http://www.ncbi.nlm.nih.gov/books?term=Gold%20AND%20micad%5Bbook%5D))
- Clinical trials (Gold nanoparticles (http://www.clinicaltrials.gov/ct2/results?term=gold+AND+nanoparticles))
- Drug information in FDA (Gold nanoparticles (http://google2.fda.gov/search?q=gold%2BAND%2Brheumatoid%2Barthritis&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=9&y=12))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Bismuth%20sulphide%20nanoparticles%20synthesis)]

AuNPs (1.9 ± 0.1 nm as determined by electron microscopy) were obtained commercially from Nanoprobes (Yaphank, NY).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Bismuth%20sulphide%20nanoparticles%20and%20in%20vitro)]

Chithrani et al. (4) showed that AuNPs of sizes between 14 and 100 nm entered cultured HeLa cells in medium containing 10% serum and trapped in vesicles in the cytoplasm as determined by transmission electron microscopy. The cellular uptake of the AuNPs increased for the first 2 h and gradually reached a plateau at 4-7 h. The uptake half life was 2.10, 1.90, and 2.24 h at a rate of 622, 1294, and 417 nanoparticles/h for the 14, 50, and 74 nm nanoparticles.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Bismuth%20sulphide%20nanoparticles%20and%20rodentia)]

In mice bearing EMT-6 syngeneic mammary tumors, AuNPs (1.9 nm, 2.7 g/kg) had a half-life of <10 min in blood after intravenous injection, followed by a slower decrease of another 50% between 15 min and 84 min (3). No AuNPs were detected in the blood by 24 h. The tissue with the highest gold accumulation was the kidneys (10.62%ID/g) at 15 min, followed by tumor (4.2%ID/g), liver (3.6%ID/g) and muscle (1.2%ID/g). The tumor/muscle ratio was 3.4 at 15 min and 9.6 at 24 h. CT imaging at 2 and 10 min showed clear delineation of blood vessels as fine as 100 μm. Imaging at later time points showed that AuNPs did not continue to concentrate in the liver but cleared through the kidneys, indicating renal excretion. Planar X-ray scan of the kidneys at 60 min revealed a detailed anatomical and functional image.

Histological examination of 24 organs and tissues from each of 15 mice injecting with 0, 7, 70 or 700 Au mg/kg showed no evidence of toxicity of in any mice (3). All mice showed normal haematology and blood chemistry at 11-30 days after injection. Mice injected with 2.7 g Au/kg survived over 1 year without any signs of sickness.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Bismuth%20sulphide%20nanoparticles%20and%20%28pig%20or%20dog%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Bismuth%20sulphide%20nanoparticles%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Bismuth%20sulphide%20nanoparticles%20and%20human)]

No publication is currently available.

## References

1 Yu S.B., Watson A.D. (1999). Metal-Based X-ray Contrast Media. Chem Rev.
2 Wallingford V.H. (1953). The development of organic iodine compounds as x-ray contrast media. J Am Pharm Assoc Am Pharm Assoc (Baltim).
3 Hainfeld J.F., Slatkin D.N., Focella T.M., Smilowitz H.M. (2006). Gold nanoparticles: a new X-ray contrast agent. Br J Radiol.
4 Chithrani B.D., Ghazani A.A., Chan W.C. (2006). Determining the size and shape dependence of gold nanoparticle uptake into mammalian cells. Nano Lett.